# 2-(+/-)-2-exo-(2'-[^18^F]Fluoro-3'-phenyl-pyridin-5'-yl)-7-azabicyclo[2.2.1]heptane

Chemical name: | 2-(+/-)-2-exo-(2'-[^18^F]Fluoro-3'-phenyl-pyridin-5'-yl)-7-azabicyclo[2.2.1]heptane
Abbreviated name: | [^18^F]FPhEP
Synonym:
Agent category: | Compound
Target: | Neuronal α4β2 nicotinic acetylcholine receptor (nAChR)
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPhEP)]

Neuronal nicotinic cholinergic receptors (nAChRs) are a heterogeneous family of ligand-gated ion channels expressed in the central nervous system, where their activation by acetylcholine and nicotine always causes a rapid increase in cellular permeability to ions, such as Na^+^ and Ca^2+^ (1-3). Nicotinic receptors exist as pentamers (homomeric or heteromeric) in various brain regions and ganglia. There are nine subtypes of ligand-binding α (α2-α10) and four subtypes of structural β (β2-β5). nAChRs have been demonstrated to be involved in cognitive processes such as learning and memory and control of movement in normal subjects. Dysfunction of nAChR has been implicated to a number of human diseases such as schizophrenia, Huntington's disease, Alzheimer's disease and Parkinson's disease. nAChRs also play a significant role in nicotine addiction.

6-[^18^F]Fluoro-A-85380 (6-[^18^F]FA (http://www.ncbi.nlm.nih.gov/books/NBK23587/)) and 2-[^18^F]FA (http://www.ncbi.nlm.nih.gov/books/NBK23401/) have been evaluated as positron emission tomography (PET) agents for the non-invasive study of α4β2 nAChR in humans (4, 5). However, prolonged imaging times (2-4 h) are required for reliable quantification because of their slow kinetics. 2-(+/-)-2-exo-(2'-Fluoro-3'-phenyl-pyridin-5'-yl)-7-azabicyclo[2.2.1]heptane (FPhEP) is a highly potent and selective α4β2 nAChR antagonist with subnanomolar affinity (6, 7). FPhEP is an analogue of epibatidine, which was showed to be a functional antagonist of α4β2 nAChR in mice. [^18^F]FPhEP is being developed as a PET agent with a faster kinetics than 2-[^18^F]FA and 6-[^18^F]FA for the non-invasive study of α4β2 nAChR in the brain.

### Related Resource Links:

- Chapters in MICAD (nACHR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=nAChR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (nAChR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=1137)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (nAChR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=Neuronal%5BAll+Fields%5D+AND+nicotinic%5BAll+Fields%5D+AND+acetylcholine%5BAll+Fields%5D+AND+receptor%5BAll+Fields%5D))
- Clinical trials (nAChR (http://www.clinicaltrials.gov/ct2/results?term=nAChR))
- Drug information in FDA (nAChR (http://google2.fda.gov/search?q=Neuronal+nicotinic+acetylcholine+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPhEP%20and%20synthesis)]

Roger et al. (7) reported synthesis of [^18^F]FPhEP by a 2-step reaction, which consisted of standard ^18^F-nucleophilic fluorination of the corresponding N-Boc-protected chloro- or bromo derivatives using microwave heating for 1.5 min and acidic deprotection of the product. An average radiochemical yield was 10-20% (non-decay corrected) with a total synthesis time of 75-80 min. Specific -activities were 2.22-3.33 GBq/μmol (60-90 mCi/μmol at end of synthesis) with a radiochemical purity of >99%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Nifene%20and%20in%20vitro)]

Roger et al. (7) reported [^18^F]FPhEP had a K_d_ value of 660 ± 75 pM and a B_max_ value of 65 ± 2 fmol/mg protein in saturation binding assays using rat brain membranes. Cytisine and nicotine (α4β2-specific ligands) exhibited good inhibition on the [^18^F]FPhEP binding with K_i_ values of 1.09 and 5.83 nM, respectively. In vitro autoradiography studies of rat brain slices indicated the highest binding of [^18^F]FPhEP in the thalamus and the lowest in the corpus callosum, consistent with α4β2 receptor distribution. Nicotine (300 μM) and FPhEP (300 μM) blocked [^18^F]FPhEP specific binding across the brain regions.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPhEP%20and%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPhEP%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPhEP%20and%20%28primate%20not%20human%29)]

Biodistribution PET study in one anesthetized baboon injected with 163 MBq (4.4 mCi, 2.1 nmol) [^18^F]FPhEP was performed by Roger et al. (7) showing a rapid accumulation of radioactivity in the brain. PET study showed selective maximal uptake in the thalamus. The cerebellum showed lower binding than the other brain regions. The peak level of 4.86% injected dose(ID)/100 ml was reached in the thalamus at 20 min. [^18^F]FPhEP radioactivity was washed out slowly in the thalamus to ~2.0% ID/100 ml at 180 min. On the other hand, injection of 430 MBq (11.6 mCi, 1.2 nmol) 2-[^18^F]FA slowly reached a peak value of 3.94% ID/100 ml at 80-90 min after injection with also a slow clearance to 3.75% ID/100 ml at 180 min. Therefore, [^18^F]FPhEP exhibited a faster kinetics than 2-[^18^F]FA.

Valette et al. (8) performed PET studies in three baboons after injection of 215 MBq (5.8 mCi, 3.3 nmol) [^18^F]FPhEP. The peak radioactivity level of 4.9 ± 0.2% ID/100 ml was reached in the thalamus at 20 min. [^18^F]FPhEP radioactivity was washed out slowly in the thalamus to 2.0 ± 0.1% ID/100 ml at 180 min. The accumulation was the lowest in the cortex. The thalamus/cerebellum ratio was 1.4 at 30 min after injection and did not increase with time. Pretreatment with nicotine, cytisine or FPhEP reduced the distribution volume (DV) values by 35% in the thalamus and 20% in the cortices, hippocampus, and putamen. The investigators concluded that [^18^F]FPhEP is not a suitable PET tracer for imaging α4β2 nAChR in the brain because nicotine failed to show substantial inhibition of [^18^F]FPhEP binding.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPhEP%20and%20human)]

No publication is currently available.

## References

1 Alkondon M., Albuquerque E.X. (2004). The nicotinic acetylcholine receptor subtypes and their function in the hippocampus and cerebral cortex. Prog Brain Res.
2 Gotti C., et al. (2006). Brain neuronal nicotinic receptors as new targets for drug discovery. Curr Pharm Des.
3 Hogg R.C., Raggenbass M., Bertrand D. (2003). Nicotinic acetylcholine receptors: from structure to brain function. Rev Physiol Biochem Pharmacol.
4 Ding Y.S., et al. (2004). 6-[18F]Fluoro-A-85380, a new PET tracer for the nicotinic acetylcholine receptor: studies in the human brain and in vivo demonstration of specific binding in white matter. Synapse.
5 Kimes A.S., et al. (2003). 2-[18F]F-A-85380: PET imaging of brain nicotinic acetylcholine receptors and whole body distribution in humans. Faseb J.
6 Huang Y., et al. (2005). Epibatidine analogues as selective ligands for the alpha(x)beta2-containing subtypes of nicotinic acetylcholine receptors. Bioorg Med Chem Lett.
7 Roger G., et al. (2006). Synthesis and radiosynthesis of [(18)F]FPhEP, a novel alpha(4)beta(2)-selective, epibatidine-based antagonist for PET imaging of nicotinic acetylcholine receptors. Bioorg Med Chem.
8 Valette H., et al. (2007). [18F]FPhEP and [18F]F2PhEP, two new epibatidine-based radioligands: evaluation for imaging nicotinic acetylcholine receptors in baboon brain. Synapse.